# [N-Methyl-^11^C]-(11β17α)-11-[4-(dimethylamino)phenyl]-17-hydroxy-21-[4-(methylsulfonyl)phenyl]-19-norpregna-4,9-dien-20-yn-3-one

Chemical name: | [N-Methyl-^11^C]-(11β17α)-11-[4-(dimethylamino)phenyl]-17-hydroxy-21-[4-(methylsulfonyl)phenyl]-19-norpregna-4,9-dien-20-yn-3-one
Abbreviated name: | [N-Methyl-^11^C]Org 34850
Synonym:
Agent Category: | Compound
Target: | Glucocorticoid receptors
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Structure of [N-methyl-^11^C]Org 34850

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=N+methyl+11C+Org+34850)]

Glucocorticoids are members of the corticosteroid family (the other members of this family are the mineralocorticoid group of compounds, which bind to the mineralocorticoid receptors (MR)) and are often used as anti-inflammatory and immunosuppressive agents for the treatment of diseases such as arthritis, asthma, and cancer, as well as inflammatory bowel disease and autoimmune diseases (1, 2). There is much evidence suggesting that glucocorticoids also have an important role in the development of stress, anxiety, and depression in rodents and humans by disturbing the hypothalamic-pituitary-adrenocortical (HPA) axis functions because these tissues have a high concentration of the glucocorticoid receptors (GR) (3). Normalization of the HPA function in humans is often observed during recovery from a depressive episode, and this has also been observed in preclinical studies with rats regardless of the type of antidepressant drug used to treat depression (4).

It has been suggested that changes in the MR/GR balance could be responsible for regulation of the psychological stress and anxiety that lead to depression. Between the two receptors, the role of GR appears to be more clear because it has been shown that GR levels are increased during periods of anxiety, and GR activity is reduced during times of low anxiety (5). Therefore, investigators in this field believe that imaging of the GR would be an excellent technique to understand the in vivo functioning and regulation of the HPA axis. Much effort has been made to develop and evaluate fluoride (^18^F)-labeled and carbon (^11^C)-labeled GR binding radiotracers to investigate the activity and function of this receptor with the use of positron emission tomography (PET) under in vivo conditions. However, studies with these radiochemicals have had little success in delineating the function of the GR because the tracers are often metabolically unstable, have shown little penetration of the blood–brain barrier, or exhibit high non-specific binding (6). The steroid compound [N-methyl-^11^C]-(11β17α)-11-[4-(dimethylamino)phenyl]-17-hydroxy-21-[4-(methylsulfonyl)phenyl]-19-norpregna-4,9-dien-20-yn-3-one ([N-methyl-^11^C]Org 34850) was reported to be a selective GR antagonist in the HPA axis with a high affinity for the receptor under in vitro conditions with the use of brain tissue homogenates (7). Because of its high potency against the GR, a ^11^C-radiolabeled version of Org 34850 was synthesized by Wuest et al. to image GR in vivo and to investigate biodistribution of the radiochemical in normal rats (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Org+34850+synthesis)]

The synthesis of [N-methyl-^11^C]Org 34850 was described by Wuest et al. (8). Briefly, [^11^C]methyl triflate was generated as described by Mock et al. (9) and used to synthesize [N-methyl-^11^C]Org 34850 from the precursor molecule Org 38665 (obtained as a gift from commercial sources). The labeled product, [N-methyl-^11^C]Org 34850, was obtained within 35 min at the end of bombardment and purified on a SPE-cartridge RP-18E. The radiochemical yield of the reaction was 23% with a purity of >98%, as determined with high-performance liquid chromatography. The specific activity of the radiotracer was reported to be 47 ± 12 GBq/μmol (1.27 ± 0.32 Ci/μmol) (n = 15 synthesis reactions) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Org+34850+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Org+34850+rodentia)]

The biodistribution of [N-methyl-^11^C]Org 34850 was studied in male Wistar rats (four animals/time point) injected with the radiochemical through the tail vein (8). The animals were euthanized 5 and 60 min after the administration of [N-methyl-^11^C]Org 34850, and the pituitary gland, the cerebellum, the rest of the brain, and all the other major glands, organs, and tissue were harvested. The accumulated radioactivity was counted, decay-corrected, and expressed as percent injected dose per gram tissue (% ID/g). Blood clearance of the radioactivity was reported to be rapid, decreasing from 0.35 ± 0.05% ID/g at 5 min after the injection to 0.16 ± 0.07% ID/g at 60 min . The pituitary and adrenal glands, which are known to express high levels of GR, showed an accumulation of 0.98 ± 0.48% ID/g and 1.62 ± 0.26% ID/g, respectively, at 5 min after tracer injection; however, at 60 min the pituitary and adrenal levels decreased to 0.23 ± 0.11% ID/g and 0.26 ± 0.10% ID/g, respectively, indicating that the radioactivity was washed out from the glands. The pancreas, liver, and brown adipose tissue showed a similar trend in the accumulation of radioactivity. A low level of radioactivity was reported to be taken up by the brain (0.09 ± 0.01% ID/g at 5 min and 0.05 ± 0.01% ID/g at 60 min), suggesting that there was some unexplained interference in the uptake of this radiochemical in the brain (8). No blocking studies were reported.

PET imaging was performed on a rat 1 h after an injection of [N-methyl-^11^C]Org 34850 through the tail vein (8). The animal was scanned for 60 min, and a review of the two-dimensional sagittal, transversal, and coronal images of the rat head revealed no uptake of the radiotracer in the brain at 60 min after administration of the radiochemical. No blocking studies were reported.

With results obtained from the biodistribution and PET studies using [N-methyl-^11^C]Org 34850, the investigators concluded that the radiotracer was not suitable for the investigation of GR in the brain (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Org+34850+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Org+34850+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Sommer P., Ray D.W. (2008). Novel therapeutic agents targeting the glucocorticoid receptor for inflammation and cancer. Curr Opin Investig Drugs.
2 Angelucci E., Malesci A., Danese S. (2008). Budesonide: teaching an old dog new tricks for inflammatory bowel disease treatment. Curr Med Chem.
3 Pariante C.M., Lightman S.L. (2008). The HPA axis in major depression: classical theories and new developments. Trends Neurosci.
4 Reus V.I., Wolkowitz O.M. (2001). Antiglucocorticoid drugs in the treatment of depression. Expert Opin Investig Drugs.
5 Rozeboom A.M., Akil H., Seasholtz A.F. (2007). Mineralocorticoid receptor overexpression in forebrain decreases anxiety-like behavior and alters the stress response in mice. Proc Natl Acad Sci U S A.
6 Steiniger B., Kniess T., Bergmann R., Pietzsch J., Wuest F.R. (2008). Radiolabeled glucocorticoids as molecular probes for imaging brain glucocorticoid receptors by means of positron emission tomography (PET). Mini Rev Med Chem.
7 Bachmann C.G., Linthorst A.C., Holsboer F., Reul J.M. (2003). Effect of chronic administration of selective glucocorticoid receptor antagonists on the rat hypothalamic-pituitary-adrenocortical axis. Neuropsychopharmacology.
8 Wuest F., Kniess T., Henry B., Peeters B.W., Wiegerinck P.H., Pietzsch J., Bergmann R. (2009). Radiosynthesis and radiopharmacological evaluation of [N-methyl-11C]Org 34850 as a glucocorticoid receptor (GR)-binding radiotracer. Appl Radiat Isot.
9 Mock B.H., Mulholland G.K., Vavrek M.T. (1999). Convenient gas phase bromination of [11C]methane and production of [11C]methyl triflate. Nucl Med Biol.